# 1-[^11^C]Arachidonic acid

Chemical name: | 1-[^11^C]Arachidonic acid
Abbreviated name: | 1-[^11^C]AA
Synonym:
Agent Category: | Small molecule
Target: | Phospholipids
Target Category: | Lipids
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - Rodents; - Non-human primates; - Humans | Structure of 1-[^11^C]arachidonic acid.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11c+arachidonic+acid)]

Arachidonic acid (AA), also known as all-cis-5,8,11,14-eicosatetraenoic acid (20:4n-6, a ω-6 fatty acid), is an essential fatty acid that is found primarily at the sn-2 position of most membrane phospholipids (PLs). Through the AA cascade it is a precursor for the synthesis of prostaglandins and leukotrienes, which have been implicated in the development of a variety of neurological disorders in mammals (1). The AA is released from the PLs by phospholipase A_2_ (PLA_2_) enzymes (both cytosolic and secretory forms) that are calcium dependent, and they are usually receptor activated. The released AA and its metabolites are believed to modulate a variety of processes in mammals including aging, ion channel functioning, neuropsychiatric disorders, inflammation, and diseases such as Alzheimer’s disease (AD) and Parkinson’s disease (2-7). Because cytokines, nitric oxide, and glutamate influence calcium mobilization in the tissue, they are known to affect PLA_2_ activation, the release of AA from PLs, and neuroinflammation observed with different neurological diseases (8-13).

The AD brain has been shown to have higher than normal PLA_2_ enzyme activity and increased levels of cytokines, β-amyloid proteins and peptides, glutamatergic markers, and AA metabolites (14-18). Esposito et al. envisioned that elevated AA metabolism in the AD brain could perhaps be used to image the neuroinflammation during the course and therapy of the disease because this fatty acid is either synthesized de novo or from linoleic acid (18:2n-6), which can be considered as its precursor in mammals (19). Using AA labeled with radioactive carbon (1-^11^C-AA), investigators have determined the regional brain AA incorporation coefficient (K*), which is the ratio of radioactivity in the brain and the integral of AA in plasma, developed using quantitative autoradiography in rodents with ^14^C-labeled AA (20) and positron emission tomography (PET) in non-human primates (21) and humans with ^11^C-labeled AA (19, 22). In addition, labeled AA has been shown to be an ideal brain imaging agent, and K* was not influenced by regional cerebral blood flow (CBF) changes measured with water containing radioactive oxygen (^15^O-water) (19).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11c+arachidonic+acid+synthesis)]

The methods described by Chang et al. (21) and Channing et al. (23) were used for the synthesis of 1-^11^C-AA (19, 22). The radiochemical was routinely obtained at the end of synthesis in ~35 min and was formulated in 0.9% saline containing 8% serum (source of the serum used was not specified) (21). Stability of the formulated tracer was not reported. Radiochemical purity of 1-^11^C-AA was reported to be >95% as determined with high-performance liquid chromatography with a specific activity of ~37 GBq/μmol (~1 Ci/μmol; n = 10) at the end of bombardment. In another publication the specific activity of 1-^11^C-AA was reported to be 3,700 MBq/μmol (100 mCi/μmol) with a radiochemical purity of >97.6% (19).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=arachidonic+acid+in+vitro)]

Much literature is available regarding AA activity under in vitro conditions (PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=arachidonic+acid+in+vitro)), however only some studies are presented in this section. Readers interested to learn more about the in vitro investigations with AA are encouraged to check references available by clicking on the above link. It is also pertinent to mention that all studies reviewed in this section were performed with unlabeled AA.

Using a mouse epidermal JB6 cell line model the effects of omega 3 fatty acids such as docosahexaenoic acid (DHA), eicosapentaenoic acid (EPA) and AA (an omega 6 fatty acid) on phorbol 12-tetradecanoate 13-acetate (TPA)- induced or epidermal growth factor (EGF) induced transcription activator protein 1 (AP-1) transactivation and the subsequent transformation of the cells was investigated (24). Among the two omega 3 fatty acids DHA was more effective at inhibiting cell transformation, but AA inhibited the beneficial effects of DHA. The investigators concluded the dietary ratio of omega 3 and omega 6 fatty acids may be an important factor in tumorigenesis under in vivo conditions.

In another study it was demonstrated that an AA metabolite (hydroxyeicosatetraenoic acid (15(S)-HETE) stimulated the adhesion of human metastatic human breast carcinoma MDA-MB-435 cells to the extracellular matrix (type IV collagen) by activating the p38 mitogen-activated protein kinase (25). This indicated that 15(S)-HETE initiated the signal transduction pathway responsible for adhesion of the cells to the extracellular matrix. AA was also shown to induce MDA-MB-231 cell migration by Navarro-Tito et. al. (26). Using tumor derived endothelial cells from human breast carcinomas it was shown that AA promotes Ca^2+^ entry into the cells during early phases of angiogenesis and this AA activity is inhibited by carboxyamidotriazole (27). This indicated that AA may have a role in angiogenesis during tumor development.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11c+arachidonic+acid+rodentia)]

Basselin et al. used autoradiography to investigate the effect of a lithium chloride (LiCl) or control diet on the K* of 1-^14^C-AA in brains of rats after an intracerebroventricular infusion of either lipopolysaccharide (LPS), which induces neuroinflammation and elevates AA metabolism in the brain, or artificial cerebrospinal fluid (aCSF) (28). Compared with animals on the aCSF diet, LPS was reported to significantly increase the K* in 28 regions of the brain in rats on the control diet. Under the same conditions, LiCl prevented an increase in K* in 18 of the same regions of the brain in rats on the control diet. LiCl was reported to increase K* in 14 regions (primarily in the visual and auditory systems) of the brain in rats fed aCSF. Markers of AA metabolism such as PLA_2_ activity as well as prostaglandin E2 and thromboxane B2 levels were increased by LPS infusion in the animals on the control diet, but no such increase was observed in rats treated with LPS and fed the LiCl diet.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11c+arachidonic+acid+non+primate+mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11c+arachidonic+acid+non+human+primates)]

The incorporation of 1-^11^C-AA was investigated using PET in the brains of normocapnic (normal carbon dioxide levels in arterial blood) and hypercapnic (increased carbon dioxide blood levels) monkeys (n = 4) (21). CBF was measured in the animals with ^15^O-water before the intravenous infusion of 1-^11^C-AA. Dynamic PET scans were performed on the animals at various time points starting at 0 min for up to 60 min after the infusion of labeled AA. During the same time, arterial blood samples were taken from the animals. The half-life of 1-^11^C-AA in the blood was reported to be 1.1 min, and radioactivity in the brain reached a steady-state within 10 min. The K* of 1-^11^C-AA was determined to be 1.1–1.2 × 10^-4^ ml/sec per gram of gray matter and remained consistent at all time points even after a 2.6-fold increase in CBF caused by hypercapnia in the animals. The investigators concluded that the incorporation of ^11^C-AA could be quantified in monkeys with PET and that the accumulation of this radiochemical in the brain was independent of blood flow.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11c+arachidonic+acid+human+studies)]

Giovacchini et al. used PET to measure the incorporation of 1-^11^C-AA in the brains of eight rested, young, and healthy adult humans (22). The K* and cerebral blood volume (V_b_) were determined for the gray and white matter in the subjects. The K* values were 5.6 ± 1.2 and 2.6 ± 0.5 μL/min per mL in the gray and white matter, respectively. The V_b_ values were reported to remain unchanged for the data analysis periods from 20 to 60 min.

In another study, the effect of healthy aging on 1-^11^C-AA incorporation, blood volume, and blood flow was investigated in eight young (27 ± 5 y) and seven old (65 ± 9 y) healthy individuals after applying the partial-volume correction (PVC) (29). No differences between the K* and V_b_ values of the young and old individuals were reported before or after the application of PVC. However, a significant reduction of CBF was apparent in the frontal cortex of individuals in the older group. After normalization to the global gray area of the brain, the K*, V_b_, and CBF values were significantly reduced in frontal lobe of the older individuals, but this difference disappeared after application of the PVC. The investigators concluded that brain function as determined with PET imaging is affected minimally by healthy aging in humans.

PET imaging was also used to study signal transduction by 1-^11^C-AA in the human brain during visual stimulation (30). 1-^11^C-AA was administered to the individuals through the intravenous route, and K* of the labeled fatty acid was determined in different parts of the brain. Sixteen healthy individuals were enrolled for the study; they were split into two groups each having eight subjects. One group was subjected to visual stimulation by flash frequencies of either 2.9 Hz or 7.8 Hz and compared with the second group, which was not visually stimulated and was kept under dark conditions (0 Hz). CBF was measured after an intravenous injection of ^15^O-water in the individuals kept under the same conditions for visual stimulation. Compared with the dark conditions, a significant increase in K* (2.3–8.9%) was observed in the Brodmann areas 17, 18, and 19 as well as in some frontal, parietal, and temporal cortical regions of the brain in individuals who were flash-stimulated at either frequency. The CBF was reported to increase significantly (3.1–22%) in these subjects, usually in areas of the brain comparable to those mentioned above. Reduced K* and CBF levels were also reported in some frontal brain areas of these individuals. From this study it was concluded AA plays a role in the signaling process provoked by visual stimulation, since visual stimulation at flash frequencies of 2.9 and 7.8 Hz compared to 0 Hz modifies both K* for AA and rCBF in visual and related areas of the human brain.

Because neuroinflammation is believed to play a role in the pathogenesis of AD, Esposito et al. used PET with 1-^11^C-AA to determine the K* for AA in patients with AD (19). Eight patients with AD (mean age, 71.7 ± 11.2 y) and nine normal control subjects (mean age, 68.7 ± 5.6 y) were enrolled in the study. CBF in the individuals was determined after an intravenous injection of ^15^O-water, and 1-^11^C-AA was administered to the individuals 15 min later to determine the K* for AA, with or without the application of PVC. Compared with the control group, the K* of global gray matter, with or without the application of PVC, was significantly elevated in subjects belonging to the AD group, but the global CBF (without the application of PVC) was reduced significantly (P < 0.05) in these individuals. The K* for AA of individuals in the AD group, after the application of PVC, was elevated in 78 of the 90 identified hemispheric gray matter regions of the brain, particularly in the neocortex, but this was not apparent in the caudate, palladium, or the thalamic regions. From these observations the investigators concluded that an upregulated AA metabolism is associated with neuroinflammation, and PET with 1-^11^C-AA can be used to detect neuroinflammation in patients with brain diseases, including AD.

## References

1 Bosetti F. (2007). Arachidonic acid metabolism in brain physiology and pathology: lessons from genetically altered mouse models. J Neurochem.
2 Calder P.C. (2008). Polyunsaturated fatty acids, inflammatory processes and inflammatory bowel diseases. Mol Nutr Food Res.
3 Hudson C., Gotowiec A., Seeman M., Warsh J., Ross B.M. (1999). Clinical subtyping reveals significant differences in calcium-dependent phospholipase A2 activity in schizophrenia. Biol Psychiatry.
4 McGahon B., Clements M.P., Lynch M.A. (1997). The ability of aged rats to sustain long-term potentiation is restored when the age-related decrease in membrane arachidonic acid concentration is reversed. Neuroscience.
5 Meves H. (2008). Arachidonic acid and ion channels: an update. Br J Pharmacol.
6 Patrick C.B., Krzywkowski P., Ramassamy C., Poirier J., Rapoport S.I., Murphy E.J. (2000). Phospholipase A2 activity is decreased selectively in the hippocampus of aged apolipoprotein E deficient mice. Neurosci Lett.
7 Smalheiser N.R., Swanson D.R. (1998). Calcium-independent phospholipase A2 and schizophrenia. Arch Gen Psychiatry.
8 Lehtonen J.Y., Holopainen J.M., Kinnunen P.K. (1996). Activation of phospholipase A2 by amyloid beta-peptides in vitro. Biochemistry.
9 Mattson M.P., Chan S.L. (2003). Neuronal and glial calcium signaling in Alzheimer's disease. Cell Calcium.
10 Orr S.K., Bazinet R.P. (2008). The emerging role of docosahexaenoic acid in neuroinflammation. Curr Opin Investig Drugs.
11 Sun G.Y., Horrocks L.A., Farooqui A.A. (2007). The roles of NADPH oxidase and phospholipases A2 in oxidative and inflammatory responses in neurodegenerative diseases. J Neurochem.
12 Rao J.S., Ertley R.N., DeMar J.C., Rapoport S.I., Bazinet R.P., Lee H.J. (2007). Dietary n-3 PUFA deprivation alters expression of enzymes of the arachidonic and docosahexaenoic acid cascades in rat frontal cortex. Mol Psychiatry.
13 Rao J.S., Ertley R.N., Lee H.J., DeMar J.C., Arnold J.T., Rapoport S.I., Bazinet R.P. (2007). n-3 polyunsaturated fatty acid deprivation in rats decreases frontal cortex BDNF via a p38 MAPK-dependent mechanism. Mol Psychiatry.
14 Farooqui A.A., Horrocks L.A. (2006). Phospholipase A2-generated lipid mediators in the brain: the good, the bad, and the ugly. Neuroscientist.
15 Jana M., Palencia C.A., Pahan K. (2008). Fibrillar amyloid-beta peptides activate microglia via TLR2: implications for Alzheimer's disease. J Immunol.
16 Kashani A., Lepicard E., Poirel O., Videau C., David J.P., Fallet-Bianco C., Simon A., Delacourte A., Giros B., Epelbaum J., Betancur C., El Mestikawy S. (2008). Loss of VGLUT1 and VGLUT2 in the prefrontal cortex is correlated with cognitive decline in Alzheimer disease. Neurobiol Aging.
17 Sanchez-Mejia R.O., Newman J.W., Toh S., Yu G.Q., Zhou Y., Halabisky B., Cisse M., Scearce-Levie K., Cheng I.H., Gan L., Palop J.J., Bonventre J.V., Mucke L. (2008). Phospholipase A2 reduction ameliorates cognitive deficits in a mouse model of Alzheimer's disease. Nat Neurosci.
18 Steinman L. (2008). Nuanced roles of cytokines in three major human brain disorders. J Clin Invest.
19 Esposito G., Giovacchini G., Liow J.S., Bhattacharjee A.K., Greenstein D., Schapiro M., Hallett M., Herscovitch P., Eckelman W.C., Carson R.E., Rapoport S.I. (2008). Imaging neuroinflammation in Alzheimer's disease with radiolabeled arachidonic acid and PET. J Nucl Med.
20 Robinson P.J., Noronha J., DeGeorge J.J., Freed L.M., Nariai T., Rapoport S.I. (1992). A quantitative method for measuring regional in vivo fatty-acid incorporation into and turnover within brain phospholipids: review and critical analysis. Brain Res Brain Res Rev.
21 Chang M.C., Arai T., Freed L.M., Wakabayashi S., Channing M.A., Dunn B.B., Der M.G., Bell J.M., Sasaki T., Herscovitch P., Eckelman W.C., Rapoport S.I. (1997). Brain incorporation of [1-11C]arachidonate in normocapnic and hypercapnic monkeys, measured with positron emission tomography. Brain Res.
22 Giovacchini G., Chang M.C., Channing M.A., Toczek M., Mason A., Bokde A.L., Connolly C., Vuong B.K., Ma Y., Der M.G., Doudet D.J., Herscovitch P., Eckelman W.C., Rapoport S.I., Carson R.E. (2002). Brain incorporation of [11C]arachidonic acid in young healthy humans measured with positron emission tomography. J Cereb Blood Flow Metab.
23 Channing M.A., Simpson N. (1993). Radiosynthesis of 1-[11C]polyhomoallylic acids. Journal of Labelled Compounds and Radiopharmaceuticals.
24 Liu G., Bibus D.M., Bode A.M., Ma W.Y., Holman R.T., Dong Z. (2001). Omega 3 but not omega 6 fatty acids inhibit AP-1 activity and cell transformation in JB6 cells. Proc Natl Acad Sci U S A.
25 Nony P.A., Kennett S.B., Glasgow W.C., Olden K., Roberts J.D. (2005). 15S-Lipoxygenase-2 mediates arachidonic acid-stimulated adhesion of human breast carcinoma cells through the activation of TAK1, MKK6, and p38 MAPK. J Biol Chem.
26 Navarro-Tito N., Robledo T., Salazar E.P. (2008). Arachidonic acid promotes FAK activation and migration in MDA-MB-231 breast cancer cells. Exp Cell Res.
27 Fiorio Pla A., Grange C., Antoniotti S., Tomatis C., Merlino A., Bussolati B., Munaron L. (2008). Arachidonic acid-induced Ca2+ entry is involved in early steps of tumor angiogenesis. Mol Cancer Res.
28 Basselin M., Villacreses N.E., Lee H.J., Bell J.M., Rapoport S.I. (2007). Chronic lithium administration attenuates up-regulated brain arachidonic acid metabolism in a rat model of neuroinflammation. J Neurochem.
29 Giovacchini G., Lerner A., Toczek M.T., Fraser C., Ma K., DeMar J.C., Herscovitch P., Eckelman W.C., Rapoport S.I., Carson R.E. (2004). Brain incorporation of 11C-arachidonic acid, blood volume, and blood flow in healthy aging: a study with partial-volume correction. J Nucl Med.
30 Esposito G., Giovacchini G., Der M., Liow J.S., Bhattacharjee A.K., Ma K., Herscovitch P., Channing M., Eckelman W.C., Hallett M., Carson R.E., Rapoport S.I. (2007). Imaging signal transduction via arachidonic acid in the human brain during visual stimulation, by means of positron emission tomography. Neuroimage.